# 4-(2-(4-(4-[^18^F]Fluoro-butyl)-phenyl)ethoxy) quinazoline

Chemical name: | 4-(2-(4-(4-[^18^F]Fluoro-butyl)-phenyl)ethoxy) quinazoline
Abbreviated name: | [^18^F]RP1003
Synonym:
Agent category: | Compound
Target: | Mitochondrial complex I (MCI)
Target category: | Enzyme
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20RP1003)]

Lipophilic cations are capable of passing through biological membranes by passive diffusion into the cytoplasm and mitochondria of cells in response to large negative plasma and mitochondrial membrane potentials. ^99m^Tc-2-Methoxyisobutylisonitrile (^99m^Tc-MIBI) and ^99m^Tc-tetrofosmin are delocalized lipophilic cations, which are rapidly taken up into cells driven by metabolic demand and membrane potential (1-4). They are used as myocardial-perfusion single-photon emission computed tomography agents and as tumor-imaging agents. However, the high accumulation of Tc tracers in the lung and liver may interfere with the detection of flow abnormalities in the myocardium. More recently, positron emission tomography (PET) imaging has emerged as an alternative approach to evaluate myocardial blood flow with the use of positron-emitting radionuclides (e.g., ^82^RbCl, ^13^NH_3_, and H_2_^15^O). However, the majority of these radiotracers exhibit short physical half-lives (<10 min). Lipophilic cations such as [^11^C]triphenylmethylphosphonium ([^11^C]TPMP) (5) and 4-[^18^F]fluorobenzyl-triphenylphosphonium ([^18^F]FBnTP) have been investigated as PET agents for myocardial and tumor imaging (6).

Mitochondrial complex I (MCI) of the mammalian electron transfer chain is composed of at least 43 protein subunits, of which seven are encoded by mitochondrial DNA (7). MC-I catalyzes the transfer of electrons from NADH to ubiquinone and translocates protons from the mitochondrial matrix to the intermembrane space to generate ATP and thus the energy supply of the cell. MC-I may also play direct roles in the mitochondrial permeability transition and in cell death pathways. Myocardium has a high mitochondrial content because of high energy usage. 4-(2-(4-(4-[^18^F]Fluoro-butyl)-phenyl)ethoxy) quinazoline ([^18^F]RP1003) has been found to be a potent MC-I inhibitor with a hydrophobic heterocyclic fenazaquin (8) and its use as a PET agent for imaging myocardium is being studied.

### Related Resource Links:

- Chapters in MICAD (MCI (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=Mitochondrial%20complex+AND+micad%5Bbook%5D))
- Gene information in NCBI (MCI (http://www.ncbi.nlm.nih.gov/gene/291))
- Articles in Online Mendelian Inheritance in Man (OMIM) (MCI (http://www.ncbi.nlm.nih.gov/entrez/dispomim.cgi?id=252010))
- Clinical trials (MCI (http://www.clinicaltrials.gov/ct2/results?term=Mitochondrial+complex+I+))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20RP1003+synthesis)]

[^18^F]RP1003 was prepared as described by Yu et al. (8). [^18^F]Fluoride/Kryptofix 2.2.2/K_2_CO_3_ and the tosylate precursor were heated in acetonitrile for 30 min at 90°C, followed by high-performance liquid chromatography purification. Total synthesis time was 90 min. Radiochemical purity was >90%, with specific activities of 27.8–55.5 GBq/µmol (0.75–1.5 Ci/µmol) at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20RP1003%20and%20in%20vitro)]

Yu et al. (8) reported that RP1003 inhibited NADH oxidation by bovine heart submitochondrial particles with a 50% inhibition concentration (IC_50_) value of 3.7 nM. The IC_50_ value of the known MC-I inhibitor rotenone was 18.2 nM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20RP1003%20and%20rodentia)]

Yu et al. (8) performed ex vivo biodistribution studies of [^18^F]RP1003 in rats (n = 10). [^18^F]RP1003 accumulated mainly in the heart, with 3.52 ± 0.36% injected dose/g (ID/g) and 2.68 ± 0.20% ID/g at 15 min and 60 min after injection, respectively. Retention of [^18^F]RP1003 in the heart was good, with some washout. The heart/blood, heart/lung, heart/liver, and heart/femur ratios were 33.5, 11.1, 1.9, and 5.8 at 60 min after injection, respectively. The uptake in the femur was 0.46% ID/g at 60 min, indicating little defluorination of [^18^F]RP1003. For comparison, heart accumulation of ^99m^Tc-sestamibi was 2.0% ID/g at 60 min, with a heart/lung ratio of 5.9 at 60 min after injection. PET imaging showed that [^18^F]RP1003 accumulated mainly in the heart and liver with low accumulation in the lung. Good myocardial images were observed at 25–35 min after injection, with little interference from the lung or liver at 55–60 min. No blocking experiment was performed. The first pass extraction efficiency was not addressed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F%20RP1003+and+(dog+or+pig+or+sheep+or+rabbit))]

Yu et al. (8) performed PET imaging studies of [^18^F]RP1003 in rabbits (n = 6). [^18^F]RP1003 accumulated mainly in the myocardium within minutes after injection, with some interference from the lung and liver at 5–15 min after injection. Retention of [^18^F]RP1003 in the heart was good and exhibited some washout, whereas the retention was much lower in the liver. Accumulation of [^18^F]RP1003 in the heart was clearly visualized at 65 min after injection, with no interference from the lung and liver accumulation of [^18^F]RP1003.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20RP1003%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20RP1003%20and%20human)]

No publication is currently available.

## References

1 Chernoff D.M., Strichartz G.R., Piwnica-Worms D. (1993). Membrane potential determination in large unilamellar vesicles with hexakis(2-methoxyisobutylisonitrile)technetium(I). Biochim Biophys Acta.
2 Chiu M.L., Kronauge J.F., Piwnica-Worms D. (1990). Effect of mitochondrial and plasma membrane potentials on accumulation of hexakis (2-methoxyisobutylisonitrile) technetium(I) in cultured mouse fibroblasts. J Nucl Med.
3 Molteni S.N., Seregni E., Botti C., Martinetti A., Ferrari L., Crippa F., Bombardieri E. (1999). The breast cancer cell line MCF7 as a model of 99mTc-SestaMIBI, 99mTc-tetrofosmin and 99mTc-Medronate incorporation. Anticancer Res.
4 Younes A., Songadele J.A., Maublant J., Platts E., Pickett R., Veyre A. (1995). Mechanism of uptake of technetium-tetrofosmin. II: Uptake into isolated adult rat heart mitochondria. J Nucl Cardiol.
5 Krause B.J., Szabo Z., Becker L.C., Dannals R.F., Scheffel U., Seki C., Ravert H.T., Dipaola A.F., Wagner H.N. (1994). Myocardial perfusion with [11C]methyl triphenyl phosphonium: measurements of the extraction fraction and myocardial uptake. J Nucl Biol Med.
6 Madar I., Ravert H.T., Du Y., Hilton J., Volokh L., Dannals R.F., Frost J.J., Hare J.M. (2006). Characterization of Uptake of the New PET Imaging Compound 18F-Fluorobenzyl Triphenyl Phosphonium in Dog Myocardium. J Nucl Med.
7 Lenaz G., Fato R., Genova M.L., Bergamini C., Bianchi C., Biondi A. (2006). Mitochondrial Complex I: structural and functional aspects. Biochim Biophys Acta.
8 Yu M., Guaraldi M., Kagan M., Mistry M., McDonald J., Bozek J., Yalamanchili P., Hayes M., Azure M., Purohit A., Radeke H., Casebier D.S., Robinson S.P. (2009). Assessment of 18F-labeled mitochondrial complex I inhibitors as PET myocardial perfusion imaging agents in rats, rabbits, and primates. Eur J Nucl Med Mol Imaging.